# Cy5.5-Ac-Cys-Z_EGFR:1907_

Chemical name: | Cy5.5-Ac-Cys-Z_EGFR:1907_
Abbreviated name: | Cy5.5-Z_EGFR:1907_
Synonym:
Agent category: | Antibody, Affibody
Target: | Epidermal growth factor receptor (EGFR, HER1)
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about EGFR.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907)]

Epidermal growth factor (EGF) is a growth factor composed of 53 amino acids (6.2 kDa) that is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with poor patient prognosis because high levels are related to increased proliferation (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). Trastuzumab is approved for clinical use for anti-cancer therapies in both Europe and North America. ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging human breast cancer (12-16). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2, based on the Z-domain residues (58 amino acids) from one of the IgG-binding domains of staphylococcal protein A, was constructed (17). Affibody molecules exhibit high binding affinity to HER2 with K_d_ values <100 pM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. The EGFR-specific Affibody Z_EGFR:1907_ (6.7 kDa) was identified to have good affinity (K_d_ = 5.4 nM) for EGFR (HER1) and was labeled with ^111^In via isothiocyanate-benzoyl-diethylenetriamine pentaacetic acid (DTPA) to form ^111^In-Bz-DTPA-Z_EGFR:1907_ (http://www.ncbi.nlm.nih.gov/books/NBK23654/) for single-photon emission computed tomography (18) imaging in nude mice bearing human tumors (19). To facilitate site-specific conjugation, Ac-Cys-Z_EGFR:1907_ (Cys at the N terminal) was synthesized and conjugated with 1,4,7,10-tetraazacyclododecane-1,4,7-tris-aceticacid-10-maleimidethylacetamide (maleimido-mono-amide-DOTA) to form Ac-Cys(DOTA)-Z_EGFR:1907_ (DOTA-Z_EGFR:1907_), and the product was labeled with ^64^Cu (t_1/2_, 12.7 h) to form ^64^Cu-DOTA-Z_EGFR:1907_ for positron emission tomography imaging studies in tumor-bearing mice (20). In this chapter, Cy5.5-Ac-Cys-Z_EGFR:1907_ (Cy5.5-Z_EGFR:1907_) was prepared and evaluated in EGFR-positive tumor in mice with specific tumor accumulation of the probe using near-infrared (NIR) fluorescence imaging (21).

### Related Resource Links:

- Chapters in MICAD (EGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/gene/1956))
- Articles in Online Mendelian Inheritance in Man (OMIM) (EGFR (http://www.ncbi.nlm.nih.gov/omim/131550))
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab), cetuximab (http://www.clinicaltrials.gov/ct2/results?term=Cetuximab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14), cetuximab (http://google2.fda.gov/search?q=Cetuximab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=7&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR+1907+synthesis)]

Ac-Cys-Z_EGFR:1907_ (6.7 kDa) was prepared with an automated solid-phase peptide synthesizer, with 10% yield and >95% purity after purification with high-performance liquid chromatography (HPLC) (21). Cy5.5-Mono-maleimide and Ac-Cys-Z_EGFR:1907_ (1.5:1 molar ratio) were incubated in phosphate buffer (pH 7.4) for 2 h at 25°C. Cy5.5-Z_EGFR:1907_ (7.7 kDa) was isolated with 47% recovery yield and >95% purity after HPLC purification. Mass spectroscopy analysis confirmed 1:1 Cy5.5conjugation. Spectrum analysis showed that Cy5.5-Z_EGFR:1907_ exhibited similar maximal fluorescence absorption (680 nm) and emission (696 nm) characteristics similar to those of free Cy5.5 dye.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20in%20vitro)]

Fluorescence microscopy analysis was performed in A431 human epidermoid carcinoma cells (high EGFR expression) and MCF7 human breast cancer cells (low EGFR expression) after incubation with 100 nM Cy5.5-Z_EGFR:1907_ for 60 min at 37°C (21). A431 exhibited intensive fluorescence signal from the cell surface and cytoplasm. Co-incubation with 100-fold excess Ac-Cys-Z_EGFR:1907_ completely abrogated the signal. On the other hand, fluorescence signal from MCF7 cells was barely visible. Cy5.5-Z_EGFR:1907_ exhibited a K_d_ value of 43.6 ± 8.4 nM for the EGFR of A431 cells, as measured with flow cytometry analysis using different doses of the probe (0.1–100 nM).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20rodentia)]

Miao et al. (21) performed NIR fluorescence imaging of nude mice (n = 3/group) bearing A431 or MCF7 tumors at 10, 30, 60, 120, and 240 min after intravenous injection of 0.5 nmol Cy5.5-Z_EGFR:1907_. The accumulation of Cy5.5-Z_EGFR:1907_ in A431 tumors could be clearly visualized from 10–240 min, with a maximum contrast at 120 min. The tumor/background ratio was 2.9 ± 0.1 at 240 min. Co-injection of Ac-Cys-Z_EGFR:1907_ (45 nmol) inhibited the tumor/background ratio to 1.8 ± 0.4 at 240 min (P < 0.05). MCF7 tumors were barely visualized, with a tumor/background ratio of 1.5 ± 0.2. Ex vivo NIR fluorescence imaging of tissues at 24 h after injection showed that the tissue with the highest signal (photons/s/cm^2^/steradian) was the kidney (1.2 × 10^8^), followed by the stomach (0.7 × 10^8^), A431 tumor (0.2 × 10^8^), and liver (0.1 × 10^8^). The spleen, heart, lung, blood, and muscle exhibited <0.03 × 10^8^ photons/s/cm^2^/steradian. The tumor/blood, tumor/muscle, tumor/lung, and tumor/liver ratios were 8, 7, 6, and 2, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=EGFR%201907%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Goldman E.R., O'Shaughnessy T.J., Soto C.M., Patterson C.H., Taitt C.R., Spector M.S., Charles P.T. (2004). Detection of proteins cross-linked within galactoside polyacrylate-based hydrogels by means of a quantum dot fluororeagent. Anal Bioanal Chem.
19 Tolmachev V., Friedman M., Sandstrom M., Eriksson T.L., Rosik D., Hodik M., Stahl S., Frejd F.Y., Orlova A. (2009). Affibody molecules for epidermal growth factor receptor targeting in vivo: aspects of dimerization and labeling chemistry. J Nucl Med.
20 Miao Z., Ren G., Liu H., Jiang L., Cheng Z. (2010). Small-animal PET imaging of human epidermal growth factor receptor positive tumor with a 64Cu labeled affibody protein. Bioconjug Chem.
21 Miao Z., Ren G., Liu H., Jiang L., Cheng Z. (2010). Cy5.5-labeled Affibody molecule for near-infrared fluorescent optical imaging of epidermal growth factor receptor positive tumors. J Biomed Opt.